# ^99m^Tc-Labeled 1-hydroxy-2-(2-isopropyl-1H-imidazole-1-yl)ethylidene-1,1-bisphosphonic acid

Chemical name: | ^99m^Tc-Labeled 1-hydroxy-2-(2-isopropyl-1H-imidazole-1-yl)ethylidene-1,1-bisphosphonic acid
Abbreviated name: | [^99m^Tc]-iPIDP
Synonym:
Agent Category: | Compound
Target: | Bone (hydroxyapatite) at low concentration; farnesyl disphosphate (pyrophosphate) synthase (molecular target) at high concentration
Target Category: | Other (Tissue); enzyme
Method of detection: | Single-photon emission computed tomography (SPECT); gamma planar imaging
Source of signal / contrast: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents; - Non-primate non-rodent mammals | Click on above structure of iPIDP for information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Bisphosphonates&cmd=DetailsSearch)]

Bisphosphonates (BPs; also known as diphosphonates) labeled with technetium ([^99m^Tc]-BPs) are often used in bone scintigraphy to detect osteoporosis and other skeletal-related events (SREs), including bone metastases (1). These chemicals are known to promote osteoclast apoptosis and have a strong affinity for hydroxyapatite, a component of the bone matrix. The mechanism of action of these bone-seeking compounds is described in detail elsewhere (2-4). Bone scintigraphy is usually performed 2–6 h after intravenous injection of a [^99m^Tc]-BP, resulting in exposure of the patient to radiation for an extended time (due to slow clearance from circulation). To develop BPs that are more efficient and require only a short waiting time before bone scintigraphy, investigators generated various BPs, such as zoledronic acid (http://www.pharma.us.novartis.com/product/pi/pdf/Zometa.pdf) (ZL), which contains an imidazole group in its structure, and evaluated their efficacy for the treatment of various bone-related diseases (5, 6). ZL was determined to be the most potent BP available for treating bone resorption and is approved by the United States Food and Drug Administration for the treatment of various tumor-induced SREs (7).

In an earlier study to further improve the potency of ZL, the imidazole group of the compound was modified to obtain 1-hydroxy-2-(2-ethyl-4-methyl-1H-imidazole-1-yl)ethane-1,1-diyldiphosphonic acid (EMIDP), and the chemical was labeled with ^99m^Tc to produce [^99m^Tc]-EMIDP (1). The biodistribution of [^99m^Tc]-EMIDP was investigated in normal mice, and the radiochemical was evaluated as a bone-imaging agent in rabbits. From these studies, the investigators concluded that [^99m^Tc]-EMIDP bound selectively to the skeletal tissue in rabbits with superior selectivity compared to that of ^99m^Tc-labeled methylene diphosphonate ([^99m^Tc]-MDP), another BP that is commonly used in the clinic. In a effort to further explore the possibility of generating a high-potency ZL derivative similar to EMIDP, Lin et al. investigated optimization of the linker chain between the imidazolyl and the germinal BP group in the structure of ZL (8). For this, a ZL derivative, 1-hydroxy-3-(1H-imidazol-1-yl)propane-1,1-diyldiphosphonic acid was synthesized and labeled with ^99m^Tc, and its biodistribution and bone-imaging properties (with single-photon emission computed tomography (SPECT) imaging) were investigated in normal mice and rabbits, respectively (8). As a continuation of this work, another ZL derivative with 2-isopropyl on the imidazole ring, 1-hydroxy-2-(2-isopropyl-1H-imidazole-1-yl)ethylidene-1,1-bisphosphonic acid (iPIDP), was prepared and labeled with ^99m^Tc (to produce [^99m^Tc]-iPIDP), and the biodistribution of the labeled compound was investigated in mice (9). In addition, the investigators used SPECT to study the bone-imaging characteristics of [^99m^Tc]-iPIDP in rabbits.

### Related Resource Links

Related chapters (http://www.ncbi.nlm.nih.gov/books/?term=MDP+AND+micad%5Bbook%5D&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books) in MICAD

Protein and mRNA sequence (http://www.ncbi.nlm.nih.gov/nuccore/NM_001037277.1) of human farnesyl diphosphate synthase

Gene information (http://www.ncbi.nlm.nih.gov/gene/2224) regarding human farnesyl diphosphate synthase (GeneID: 2224)

Farnesyl diphosphate synthase in Online Mendelian Inheritance in Man (OMIM) (http://www.ncbi.nlm.nih.gov/omim/134629)

Structure of farnesyl diphosphate synthase (http://www.ncbi.nlm.nih.gov/Structure/mmdb/mmdbsrv.cgi?uid=59201) complexed with a bisphosphonate

Farnesyl diphosphate synthase in Kyoto Encyclopedia of Genes and Genomes (KEGG) Pathways (http://www.genome.jp/dbget-bin/www_bget?pathway+hsa00900)

Clinical trials (http://clinicaltrials.gov/ct2/results?term=bisphosphonates) with bisphosphonates (or diphosphonates)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=1-hydroxy-2-%282-isopropyl-1H-imidazole-1-yl%29%20ethylidene-1%2C1-bisphosphonic%20synthesis&cmd=DetailsSearch)]

The synthesis and ^99m^Tc labeling of iPIDP has been described by Wang et al. (9). The radiochemical purity (RCP) of [^99m^Tc]-iPIDP was reported to be >95%. The radiochemical yield (RCY) and specific activity of the labeled compound was not reported.

In one of the studies, ^99m^Tc-labeled ZL ([^99m^Tc]-ZL) was also used for comparison purposes, but the RCY, RCP, and specific activity of this labeled compound were not reported (9).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=iPIDP%20in%20vitro%20studies%5ball%5d&cmd=correctspelling)]

The in vitro stability of [^99m^Tc]-iPIDP was investigated by incubating the radiolabeled compound for 6 h at room temperature in phosphate buffered saline (pH 4.0-6.0), and the RCP of the tracer was evaluated every 0.5 h with paper chromatography (9). At the end of the 6-h incubation, the RCP of [^99m^Tc]-iPIDP was reported to be 96.6 ± 0.3%. This indicated that the tracer was stable at room temperature for at least 6 h.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=99mTc-iPIDP%20rodentia&cmd=DetailsSearch)]

Wang et al. investigated the biodistribution of [^99m^Tc]-iPIDP in Institute of Cancer Research mice (9). The animals (n = 5 mice/group) were injected with freshly prepared [^99m^Tc]-iPIDP through the lateral tail vein, and the mice were euthanized at predetermined time points from 5 min to 240 min (4 h) postinjection (p.i.) to determine the amount of radioactivity accumulated in the major organs, including bone. Data from the study were presented as percent uptake of injected dose per gram tissue (% ID/g). The bone showed an accumulation of 3.96 ± 0.37% ID/g at 5 min p.i., which increased to 9.63 ± 0.64% ID/g at 60 min p.i. and decreased to 4.57 ± 0.14% ID/g at 240 min p.i. Among the other organs, the kidneys showed the highest uptake with 10.01 ± 0.68% ID/g at 5 min p.i., which decreased to 1.39 ± 0.01% ID/g at 240 min p.i. A similar trend in the uptake of radioactivity was observed in the other non-target organs. The bone/organ uptake ratios for muscle, spleen, brain, lung, heart, and liver were 12.19, 15.32, 95.55, 3.32, 8.78, and 11.22, respectively, at 15 min p.i. and increased to 67.83, 73.91, 429.06, 24.02, 66.00, and 37.45, respectively, at 60 min p.i. This indicated that accumulation of radioactivity in the soft tissue was low compared to the bone and that it was cleared rapidly from the soft tissues. No blocking studies were reported.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=99mTc-iPIDP%20rabbit&cmd=DetailsSearch)]

For bone imaging, a New Zealand white rabbit (under anesthesia) was injected with [^99m^Tc]-iPIDP through the marginal ear vein, and dynamic images of the animal were acquired every 5 min for the next 60 min. This was followed by the acquisition of static images every hour for 4 h (9). From the images it was clear that radioactivity in the animals was present selectively in the bones, and a low amount of the tracer was present in the various soft tissues, except in the kidneys and the bladder. These results were consistent with observations made during the biodistribution studies and showed that the radioactivity was cleared from circulation primarily through the urinary route.

For comparison with [^99m^Tc]-iPIPD, dynamic bone images were also acquired from a New Zealand white rabbit injected with [^99m^Tc]-ZL as described above (9). Images obtained with [^99m^Tc]-ZL showed that both tracers had similar biodistribution patterns in the bones and the soft tissues. However, compared to [^99m^Tc]-iPIPD, with [^99m^Tc]-ZL there was a significantly higher (P value not reported) accumulation of radioactivity in the liver at the various time points.

Static images acquired from the animals with the two tracers showed that the rabbit skeleton was clearly visible with both [^99m^Tc]-iPIPD and [^99m^Tc]-ZL at 1 h p.i (9). A comparison of the images obtained with the two radiochemicals showed that with [^99m^Tc]-iPIPDuptake of radioactivity by the liver was significantly lower than that with [^99m^Tc]-ZL. Even at 4 h p.i., the liver was clearly visible with [^99m^Tc]-ZL, indicating that the clearance of this tracer from the organ was more gradual than that of [^99m^Tc]-iPIPD.

From these studies, the investigators concluded that [^99m^Tc]-iPIPD was a promising agent for bone imaging in animals; however, further studies are necessary before it can be used in the clinic (9).

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=99mTc-iPIDP%20Non-Human%20Primates&cmd=DetailsSearch)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=99mTc-iPIDP%20Human%20Studies)]

No publication is currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Lin J., Luo S., Chen C., Qiu L., Wang Y., Cheng W., Ye W., Xia Y. (2010). Preparation and preclinical pharmacological study on a novel bone imaging agent (99m)Tc-EMIDP. Appl Radiat Isot.
2 Kimmel D.B. (2007). Mechanism of action, pharmacokinetic and pharmacodynamic profile, and clinical applications of nitrogen-containing bisphosphonates. J Dent Res.
3 Zhang Y., Cao R., Yin F., Hudock M.P., Guo R.T., Krysiak K., Mukherjee S., Gao Y.G., Robinson H., Song Y., No J.H., Bergan K., Leon A., Cass L., Goddard A., Chang T.K., Lin F.Y., Van Beek E., Papapoulos S., Wang A.H., Kubo T., Ochi M., Mukkamala D., Oldfield E. (2009). Lipophilic bisphosphonates as dual farnesyl/geranylgeranyl diphosphate synthase inhibitors: an X-ray and NMR investigation. J Am Chem Soc.
4 Mitterhauser M., Toegel S. (2011). Radiopharmaceutical considerations on bone seeker uptake: should we learn from therapeutical targets of bisphosphonates?. Nucl Med Biol.
5 Widler L., Jaeggi K.A., Glatt M., Muller K., Bachmann R., Bisping M., Born A.R., Cortesi R., Guiglia G., Jeker H., Klein R., Ramseier U., Schmid J., Schreiber G., Seltenmeyer Y., Green J.R. (2002). Highly potent geminal bisphosphonates. From pamidronate disodium (Aredia) to zoledronic acid (Zometa). J Med Chem.
6 Asikoglu M., Durak F.G. (2009). The rabbit biodistribution of a therapeutic dose of zoledronic acid labeled with Tc-99m. Appl Radiat Isot.
7 Smith M.R. (2008). Osteoclast targeted therapy for prostate cancer: bisphosphonates and beyond. Urol Oncol.
8 Lin J., Qiu L., Cheng W., Luo S., Ye W. (2011). Preparation and in vivo biological investigations on a novel radioligand for bone scanning: technetium-99m-labeled zoledronic acid derivative. Nucl Med Biol.
9 Wang Y., Luo S., Lin J., Qiu L., Cheng W., Zhai H., Nan B., Ye W., Xia Y. (2011). Animal studies of 99mTc-i-PIDP: a new bone imaging agent. Appl Radiat Isot.